# 5-[^123^I]Iodo-3-[2(S)-2-azetidinylmethoxy]pyridine

Chemical name: | 5-[^123^I]Iodo-3-[2(S)-2-azetidinylmethoxy]pyridine
Abbreviated name: | 5-[^123^I]IA
Synonym: | 5-[^123^I]Iodo-A-85380
Agent Category: | Compound
Target: | Neuronal α4β2 nicotinic acetylcholine receptor (nAChR)
Target Category: | Receptor binding
Method of detection: | SPECT, planar
Source of signal: | ^123^I
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20A-85380)]

Neuronal nicotinic cholinergic receptors (nAChRs) are a heterogeneous family of ligand-gated ion channels expressed in the central nervous system, where their activation by acetylcholine and nicotine always causes a rapid increase in cellular permeability to ions, such as Na^+^ and Ca^2+^ (1-3). Nicotinic receptors exist as pentamers (homomeric or heteromeric) in various brain regions and ganglia. There are nine subtypes of ligand-binding α (α2-α10) and four subtypes of structural β (β2-β5) receptors. nAChRs have been to be involved in cognitive processes such as learning memory and control of movement in normal subjects. Dysfunction of nAChR has been implicated to a number of human diseases such as schizophrenia, Huntington's disease, Alzheimer's disease (AD) and Parkinson's disease. nAChRs also play a significant role in nicotine addiction and other health problems associated with tobacco smoking.

3-[2(S)-2-Azetidinylmethoxy]pyridine (A-85380) is a highly potent and selective α4β2 nAChR agonist with subnanomolar affinity (4, 5). 6-[^18^F]Fluoro-A-85380 and 2-[^18^F]fluoro-A-85380 have been studied in humans as PET agents for α4β2 nAChR imaging in the brain. A-85380 has also been labeled as 5-[^123^I]iodo-3-[2(S)-2-azetidinylmethoxy]pyridine (5-[^123^I]iodo-A-85380). 5-[^123^I]iodo-A-85380 (5-[^123^I]IA) is being developed as a single photon emission computed tomography (SPECT) agent for the non-invasive study of nAChR in the brain.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20A-85380%20and%20synthesis)]

Horti et al. (6) reported synthesis of 5-[^123^I]IA by a two-step procedure, which consisted of standard chloramine-T oxidative radioiodination of 5-trimethylstannyl-3-[1-tert-butoxycarbonyl-2(S)-azetidinyl)methoxy]pyridine and acidic deprotection of the product. Average radiochemical yields were 40-55% (end of synthesis). The average specific activity was 259 GBq/μmol (7 Ci/μmol at end of synthesis) with a radiochemical purity of >95%. Musachio et al. (7) reported a similar synthesis of 5-[^123^I]IA with a radiochemical yield of up to 52% and specific activities of >320 GBq/μmol (>8.5 Ci/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20A-85380%20and%20in%20vitro)]

Sullivan et al. (5) reported that A-85380 had inhibition constant (K_i_) values of 0.05 ± 0.01, 148 ± 13, and 314 ± 12 nM in human α4β2, α7, and muscle α1β1δγ receptors, respectively. A-85380 (up to 10,000 nM) has no effect in other neurotransmitter binding assays. Horti et al. (6) determined that 5-[^123^I]IA had a K_d_ (affinity constant) of 11.2 ± 0.3 pM and a B_max_ (receptor density) of 134 ± 2 fmol/mg protein in rat forebrain homogenates. Saji et al. (8) reported that 5-IA, cytisine and nictotine had K_i_ values (obtained by use of 5-[^125^I]IA) of 0.40, 1.40 and 1.32 pM for α4β2 in rat brain membranes, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20A-85380%20and%20rodentia)]

Saji et al. (8) reported biodistribution studies of 5-[^125^I]IA in the rats, showing peak accumulation in the brain (1.05% injected dose/g(ID/g)) at 60 min. The kidney had the highest accumulation (5.09% ID/g), followed by the liver (1.55% ID/g), thyroid (0.44% ID/g), and heart (0.19% ID/g). All organs showed washout with time except the thyroid, which had a gradual increase to 2.35% ID/g at 180 min. The highest accumulation of radioactivity was observed in the thalamus (1.5% ID/g), followed by the cortex (1.2% ID/g), striatum (1.0% ID/g), and cerebellum (0.7% ID/g) at 60 min after injection of 5-[^125^I]IA. Nicotine and cytisine pretreatments significantly inhibited 5-[^125^I]IA binding in all regions of the brain, including the cerebellum. Scopolamine (a muscarinic AChR antagonist) did not exhibit any inhibition. Pretreatment with 5-IA (300 nmol/kg) blocked accumulation in the thalamus and cortex by 90% at 60 min and to a lesser extent in the cerebellum. The fraction of unchanged 5-[^125^I]IA in plasma was 60, 18, 13 and 3% at 5, 15, 30 and 60 min, respectively. Two hydrophilic metabolites were detected. The fraction of unchanged 5-[^125^I]IA in the brain was 90% at 60 min.

Vaupel et al. (9) performed biodistribution studies in mice after injection of 0.11 MBq (3 μCi) 5-[^125^I]IA (0.05 nmol/kg). 5-[^125^I]IA accumulation was higher in the thalamus (10% ID/g) and superior colliculus (10% ID/g) and lower in the cerebellum (2% ID/g) at 60 min after injection. The cortex, hippocampus and striatum had an intermediate level of uptake of 4-5% ID/g. A peak uptake was reached in the cerebellum at <5 min (earlier than most other brain regions), followed by a rapid washout. The thalamus/cerebellum ratio increased from 5 at 60 min to 37 at 240 min. Nicotine and cytisine pretreatments significantly inhibited 5-[^125^I]IA binding in all regions of the brain, with little inhibition in the cerebellum. Scopolamine did not exhibit any inhibition. Pretreatment with 5-IA (300 nmol/kg) blocked accumulation in the thalamus and cortex by >85%. Only marginal inhibition was observed in the cerebellum.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20A-85380%20and%20(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20A-85380%20and%20(primate%20not%20human))]

5-[^123^I]IA SPECT studies with non-human primates showed substantial brain accumulation with selective maximal uptake in the regions of the thalamus and intermediate uptake in the striatum and cortex (7, 10, 11). The cerebellum showed lower binding than the other brain regions. 5-[^123^I]IA radioactivity was blocked (pretreatment) and displaced (injected after tracer) by A-85380, nicotine and cytisine. Using the one-tissue compartment model, Fujita et al. (11) estimated total distribution volume (V_T_’)values of 24.5–35.1 and 7.6-16.7 in the thalamus and cerebellum, respectively, of three baboons. Cytisine (0.8 and 1.0 mg/kg) showed displacement of 5-[^123^I]IA in the thalamus (70-72%) and cerebellum (36-55%) when administered less than 2 h after 5-[^123^I]IA injection. Therefore, the cerebellum is not suitable to be used as a receptor-poor region. The fraction of unchanged 5-[^123^I]IA in the plasma as determined by high-performance liquid chromatography (HPLC was 20-26% at 30 min after injection.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%5BAll%20Fields%5D%20AND%20%28%225-iodo-3-%282-azetidinylmethoxy%29pyridine%22%5BSubstance%20Name%5D%20OR%205-IA-85380%5BText%20Word%5D%29%20AND%20%28%28%22humans%22%5B)]

Fujita et al. (12) performed SPECT studies in six healthy nonsmoking subjects (age 33 ±15 years) with injection of 317 ± 42 MBq (8.6 ± 1.1 mCi) 5-[^123^I]IA. The study duration was 5-8 h. Nonlinear least-squares compartmental analysis was applied to calculate total (V_T_') and specific (V_S_') distribution volumes. V_T_' was well identified by both one- and two-tissue compartment models, with a coefficient of variation of <5% in most regions. The two-compartment model estimated V_T_' values of 51, 32, 27, 22, 20, 20, 19, and 17 ml/cm^3^ in the thalamus, pons, putamen, cerebellum, frontal cortex, temporal cortex, parietal cortex, and occipital cortex, respectively. SPECT studies were also performed on the same six subjects with a bolus plus constant infusion (B/I) (total dose: 331 ± 55 MBq, 8.9 ± 1.5 mCi). B/I studies did not provide accurate assessment of V_T_' values because of deviations from equilibrium conditions as a result of variable B/I ratio. Later, Staley et al. (13) and Mamede et al. (14) reported reproducible and reliable results were obtained using B/I equilibrium imaging by using constant B/I ratio and 2-compartment model with graphical analyses in healthy nonsmoking subjects.

Human dosimetry of 5-[^123^I]IA was estimated in ten normal volunteers (five males and five females) by Fujita et al. (15). Dynamic whole-body PET scans were acquired after the injection of 98 ± 6 MBq (2.65 ± 0.16 mCi, 0.53 ± 0.03 nmol) of 5-[^123^I]IA. There were no reported pharmacological effects associated with the 5-[^123^I]IA dosages. Uptake of 5-[^123^I]IA in the brain reached a peak of 5.0%ID within 14 min after injection. The greatest accumulation of 5-[^123^I]IA was in the thalamus, followed by the midbrain and pons. About 50% ID was excreted in urine in 8 h. The organ with the highest absorbed dose was found to be the urinary bladder (140 µGy/MBq (518 mrad/mCi)), followed by the lower large intestine wall (72 µGy/MBq (266 mrad/mCi)), upper large intestine wall (64 µGy/MBq (237 mrad/mCi)), kidney (54 µGy/MBq (199 mrad/mCi)), and liver (45 µGy/MBq (167 mrad/mCi)). The effective dose equivalent was calculated to be 32 µSv/MBq (0.12 rem/mCi). Ueda et al. (16) estimated the effective dose equivalent to be 30 µSv/MBq (0.11 rem/mCi) in another study of healthy volunteers.

## Supplemental Information

[Disclaimers]

Synthesis Protocol

Toxicology

Preclinical Pharmacology

Clinical Pharmacology

Animal Dosimetry

Human Dosimetry

## References

1 Alkondon M., Albuquerque E.X. (2004). The nicotinic acetylcholine receptor subtypes and their function in the hippocampus and cerebral cortex. Prog Brain Res.
2 Gotti C., Riganti L., Vailati S., Clementi F. (2006). Brain neuronal nicotinic receptors as new targets for drug discovery. Curr Pharm Des.
3 Hogg R.C., Raggenbass M., Bertrand D. (2003). Nicotinic acetylcholine receptors: from structure to brain function. Rev Physiol Biochem Pharmacol.
4 Abreo M.A., Lin N.H., Garvey D.S., Gunn D.E., Hettinger A.M., Wasicak J.T., Pavlik P.A., Martin Y.C., Donnelly-roberts D.L., Anderson D.J., Sullivan J.P., Williams M., Arneric S.P., Holladay M.W. (1996). Novel 3-Pyridyl ethers with subnanomolar affinity for central neuronal nicotinic acetylcholine receptors. J Med Chem.
5 Sullivan J.P., Donnelly-Roberts D., Briggs C.A., Anderson D.J., Gopalakrishnan M., Piattoni-Kaplan M., Campbell J.E., McKenna D.G., Molinari E., Hettinger A.M., Garvey D.S., Wasicak J.T., Holladay M.W., Williams M., Arneric S.P. (1996). A-85380 [3-(2(S)-azetidinylmethoxy) pyridine]: in vitro pharmacological properties of a novel, high affinity alpha 4 beta 2 nicotinic acetylcholine receptor ligand. Neuropharmacology.
6 Horti A.G., Koren A.O., Lee K.S., Mukhin A.G., Vaupel D.B., Kimes A.S., Stratton M., London E.D. (1999). Radiosynthesis and preliminary evaluation of 5-[123/125I]iodo-3-(2(S)-azetidinylmethoxy)pyridine: a radioligand for nicotinic acetylcholine receptors. Nucl Med Biol.
7 Musachio J.L., Villemagne V.L., Scheffel U.A., Dannals R.F., Dogan A.S., Yokoi F., Wong D.F. (1999). Synthesis of an I-123 analog of A-85380 and preliminary SPECT imaging of nicotinic receptors in baboon. Nucl Med Biol.
8 Saji H., Ogawa M., Ueda M., Iida Y., Magata Y., Tominaga A., Kawashima H., Kitamura Y., Nakagawa M., Kiyono Y., Mukai T. (2002). Evaluation of radioiodinated 5-iodo-3-(2(S)-azetidinylmethoxy)pyridine as a ligand for SPECT investigations of brain nicotinic acetylcholine receptors. Ann Nucl Med.
9 Vaupel D.B., Mukhin A.G., Kimes A.S., Horti A.G., Koren A.O., London E.D. (1998). In vivo studies with [125I]5-I-A-85380, a nicotinic acetylcholine receptor radioligand. Neuroreport.
10 Chefer S.I., Horti A.G., Lee K.S., Koren A.O., Jones D.W., Gorey J.G., Links J.M., Mukhin A.G., Weinberger D.R., London E.D. (1998). In vivo imaging of brain nicotinic acetylcholine receptors with 5-[123I]iodo-A-85380 using single photon emission computed tomography. Life Sci.
11 Fujita M., Tamagnan G., Zoghbi S.S., Al-Tikriti M.S., Baldwin R.M., Seibyl J.P., Innis R.B. (2000). Measurement of alpha4beta2 nicotinic acetylcholine receptors with [123I]5-I-A-85380 SPECT. J Nucl Med.
12 Fujita M., Ichise M., van Dyck C.H., Zoghbi S.S., Tamagnan G., Mukhin A.G., Bozkurt A., Seneca N., Tipre D., DeNucci C.C., Iida H., Vaupel D.B., Horti A.G., Koren A.O., Kimes A.S., London E.D., Seibyl J.P., Baldwin R.M., Innis R.B. (2003). Quantification of nicotinic acetylcholine receptors in human brain using [123I]5-I-A-85380 SPET. Eur J Nucl Med Mol Imaging.
13 Staley J.K., van Dyck C.H., Weinzimmer D., Brenner E., Baldwin R.M., Tamagnan G.D., Riccardi P., Mitsis E., Seibyl J.P. (2005). 123I-5-IA-85380 SPECT measurement of nicotinic acetylcholine receptors in human brain by the constant infusion paradigm: feasibility and reproducibility. J Nucl Med.
14 Mamede M., Ishizu K., Ueda M., Mukai T., Iida Y., Fukuyama H., Saga T., Saji H. (2004). Quantification of human nicotinic acetylcholine receptors with 123I-5IA SPECT. J Nucl Med.
15 Fujita M., Seibyl J.P., Vaupel D.B., Tamagnan G., Early M., Zoghbi S.S., Baldwin R.M., Horti A.G., Kore N.A., Mukhin A.G., Khan S., Bozkurt A., Kimes A.S., London E.D., Innis R.B. (2002). Whole-body biodistribution, radiation absorbed dose, and brain SPET imaging with [123i]5-i-A-85380 in healthy human subjects. Eur J Nucl Med Mol Imaging.
16 Ueda M., Iida Y., Mukai T., Mamede M., Ishizu K., Ogawa M., Magata Y., Konishi J., Saji H. (2004). 5-[123I]Iodo-A-85380: assessment of pharmacological safety, radiation dosimetry and SPECT imaging of brain nicotinic receptors in healthy human subjects. Ann Nucl Med.